# ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinic acid-cyclo(Arg-Gly-Asp-D-Try-Lys)

Chemical name: | ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinic acid-cyclo(Arg-Gly-Asp-D-Try-Lys)
Abbreviated name: | ^99m^Tc-EDDA/HYNIC-c(RGDyK), ^99m^Tc-EDDA/HYNIC-RGD, ^99m^Tc-HYNIC-RGD
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Hydrazinonicotinic acid (HYNIC) is a coupling agent for ^99m^Tc labeling of peptides that can achieve high specific activities without affecting the receptor-binding ability of the amino acid sequence. Decristoforo et al. (13) reported the success of radiolabeling cyclo(Arg-Gly-Asp-D-Tyr-Lys) (c(RGDyK)) by conjugation of HYNIC to the ε amino group of Lys with ethylenediaminediacetic acid (EDDA) and tris(hydroxymethyl)-methylglycine (tricine) as coligand. The ^99m^Tc-EDDA/HYNIC-c(RGDyK) peptide showed high tumor accumulation in nude mice bearing M21 human melanoma tumors and A549 human lung carcinoma tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+synthesis)]

Decristoforo et al. (13) reported the synthesis of ^99m^Tc-EDDA/HYNIC-c(RGDyK) by the tricine/EDDA exchange labeling method. In brief, 0.01 mg HYNIC-c(RGDyK) was incubated with EDDA/tricine solution (20 mg/ml tricine, 10 mg/ml EDDA), 800 MBq (21.62 mCi) ^99m^TcO_4_−, and stannous chloride (1 mg/ml) in a total volume of ~2 ml (pH 6–7) for 10 min at 100ºC. Radiochemical purity was >95% after Sep-Pak purification with a specific activity of ~100 GBq/μmol (2.7 Ci/μmol). The conjugation efficiency was 93.9%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+in+vitro)]

Decristoforo et al. (13) performed in vitro binding studies of HYNIC-c(RGDyK) in cultured M21 human melanoma cells with ^125^I-echistatin. HYNIC-c(RGDyK) had an inhibition concentration (IC_50_) value of 6.0 nM. Cellular uptake of ^99m^Tc-EDDA/HYNIC-c(RGDyK) was 1.25%/mg protein for α_v_β_3_ receptor–positive M21 cells and 0.1%/mg protein for receptor-negative M21L cells for 90 min at 37ºC. The uptake in M21 cells was reduced to 0.1%/mg protein by excess c(RGDyK).

The in vitro stability of ^99m^Tc-EDDA/HYNIC-c(RGDyK) purified by solid-phase extraction was tested by incubating the radiolabeled peptide (200–1,000 pmol/ml) in a phosphate buffer solution that contained a 10,000-fold molar excess of cysteine, histidine, or fresh human plasma for up to 24 h at 37ºC as well as in kidney or liver homogenates for up to 2 h at 37ºC. No significant degradation of ^99m^Tc-EDDA/HYNIC-c(RGDyK) was observed under any of these conditions. Less than 5% of ^99m^Tc-EDDA/HYNIC-c(RGDyK) was bound to human plasma protein for up to 6 h at 37ºC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+rodentia)]

Decristoforo et al. (13) performed biodistribution studies of ^99m^Tc-EDDA/HYNIC-c(RGDyK) in nude mice bearing M21 or M21L tumors. The initial tracer accumulation in the α_v_β_3_ integrin–expressing M21 tumor was 2.73 ± 0.26% injected dose per gram (ID/g) at 1 h and decreased to 2.06 ± 0.37% ID/g at 4 h. The highest concentration of radioactivity was found in the kidney (3.68% ID/g), followed by the liver (2.63% ID/g), stomach (2.50% ID/g), and intestine (2.04% ID/g) at 1 h. Blood levels were 0.98% ID/g at 1 h and 0.45% ID/g at 4 h. The ^99m^Tc-EDDA/HYNIC-c(RGDyK) accumulation in the α_v_β_3_ receptor–negative M21L tumor was 0.85 ± 0.20% ID/g at 1 h, which was lower than that in the M21 tumor. The radioactivity levels in other organs were similar to those of mice bearing M21 tumors. Single-photon emission computed tomography gamma planar imaging was performed in mice bearing A549 tumors 4 h after injection of 37 MBq (1 mCi, 1 μg) of ^99m^Tc-EDDA/HYNIC-c(RGDyK). The urinary bladder exhibited the highest accumulation of radioactivity, followed by the liver and kidney. The tumor was clearly seen with an uptake value of 4.92%, which was reduced to 0.88% by co-injection of c(RGDyK) (100 μg).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Decristoforo C., Faintuch-Linkowski B., Rey A., von Guggenberg E., Rupprich M., Hernandez-Gonzales I., Rodrigo T., Haubner R. (2006). [99mTc]HYNIC-RGD for imaging integrin alphavbeta3 expression. Nucl Med Biol.